# ^89^Zr-Labeled N-succinyldesferrioxamine-ranibizumab

Chemical name: | ^89^Zr-Labeled N-succinyldesferrioxamine-ranibizumab
Abbreviated name: | [^89^Zr]-Ranibizumab
Synonym:
Agent Category: | Antibody
Target: | Vascular endothelial growth factor-A (VEGF-A)
Target Category: | Antigen
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^89^Zr
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ranibizumab&cmd=DetailsSearch)]

The vascular endothelial growth factors (VEGF) are a family of mitogenic glycoproteins (designated VEGF-A thru VEGF-E) that promote angiogenesis by the activation of the VEGF receptors (VEGFR) via a tyrosine kinase (TK) signaling pathway. These growth factors are known to assist in the survival and promotion of malignant tumors by increasing the abnormal neovascularization of the lesions (1). As a result, anti-angiogenic therapy with bevacizumab (http://dailymed.nlm.nih.gov/dailymed/drugInfo.cfm?id=35213&CFID=15276089&CFTOKEN=bb49a22e29ea7208-F1D430F6-0BDF-7F7C-4CB8CE15E220DA04&jsessionid=ca304feb6e17227c5918), a humanized anti-VEGF monoclonal antibody (mAb), its Fab fragment ranibizumab (http://dailymed.nlm.nih.gov/dailymed/drugInfo.cfm?id=19541&CFID=15276089&CFTOKEN=bb49a22e29ea7208-F1D430F6-0BDF-7F7C-4CB8CE15E220DA04&jsessionid=ca304feb6e17227c5918), and small molecule VEGFR TK inhibitors such as sorafenib (http://dailymed.nlm.nih.gov/dailymed/drugInfo.cfm?id=32493&CFID=15276089&CFTOKEN=bb49a22e29ea7208-F1D430F6-0BDF-7F7C-4CB8CE15E220DA04&jsessionid=ca304feb6e17227c5918) and sunitinib (http://dailymed.nlm.nih.gov/dailymed/drugInfo.cfm?id=19678&CFID=15276089&CFTOKEN=bb49a22e29ea7208-F1D430F6-0BDF-7F7C-4CB8CE15E220DA04&jsessionid=ca304feb6e17227c5918#nlm34089-3) are often used to treat various types of cancer (2) and other VEGF-related health conditions (3). However, these therapies are not entirely effective due to the development of resistance to the treatments as discussed in detail elsewhere (4). In addition, the efficacy of an anti-angiogenic therapy cannot be reliably assessed with either invasive (e.g., biopsy to measure different histochemical vascular markers) or non-invasive (imaging with [^15^O]H_2_O, ultrasound, optical probes, or magnetic resonance) methods (4). Radiolabeled VEGF or anti-VEGFR antibodies have been used to study the VEGF/VEGFR expression profiles of angiogenic tumors with single-photon emission computed tomography or positron emission tomography (PET) imaging in preclinical studies; however, because the expression level of these molecules in the tumor changes with the tumor's development stage, data obtained from these studies often yields inconclusive results (4).

PET imaging with ^89^Zr-labeled bevacizimab (^89^Zr-bevacizimab; molecular weight ((mol. wt.) ~150 kDa) was recently shown to be suitable for the determination of VEGF levels in xenograft tumors on athymic nude mice and to predict tumor response to VEGF-dependent anti-angiogenic therapy (5). The physical half-life of ^89^Zr is ~78.5 h. The main limitation of this imaging agent is its long circulating serum half-life (21 days), and the maximum signal was observed only 4–7 days postinjection (p.i.) of the radiolabeled mAb. In an effort to develop an imaging agent superior to ^89^Zr-bevacizimab to predict the effectiveness of anti-VEGF therapy, ranibizumab (mol. wt. ~40 kDa) was labeled with ^89^Zr (^89^Zr-ranibizumab). For the development, characteristics, and clinical application of ranibizumab, see Ferrara et al. (6). The biodistribution and possible utility of ^89^Zr-ranibizumab as a tumor-imaging agent to determine the efficacy of sunitinib was investigated in athymic mice bearing SKOV-3 (a human adenocarcinoma cell line), A2780 (a human ovarian cancer cell line), or Colo205 (a human colorectal adenocarcinoma cell line) xenograft tumors (7).

### Other Sources of Information

Other VEGF (or related) chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=VEGF%20AND%20micad%5Bbook%5D)

Chapters on anti-angiogenic agents (http://www.ncbi.nlm.nih.gov/books/?term=anti-angiogenic%20AND%20micad%5Bbook%5D) in MICAD

Human VEGF-A protein sequence and mRNA transcript variant 1 (http://www.ncbi.nlm.nih.gov/nuccore/NM_001025366?) (gene ID: 7422)

VEGF-A in OMIM (http://www.ncbi.nlm.nih.gov/omim?term=vegf) (Online Mendelian Inheritance in Man)

VEGF related clinical trials (http://clinicaltrials.gov/ct2/results?term=VEGF)

VEGF pathways (http://pid.nci.nih.gov/search/pathway_landing.shtml?pathway_id=100006&pathway_name=vegf%20hypoxia%20and%20angiogenesis&source=BioCarta%20Imported&what=graphic&jpg=on&ppage=1) related to hypoxia and angiogenesis (from NCI/Nature Pathways Interaction Database)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-ranibizumab%20synthesis&cmd=DetailsSearch)]

The source and ^89^Zr-labeling of ranibizumab was performed as described by Nagengast et al. (7). The radiochemical yield (RY) of ^89^Zr-ranibizumab was >95%, and the specific activity (SA) of the final product was 1,500 MBq/mg (40.5 mCi/mg). The radiochemical purity (RP) of the labeled mAb was not reported. ^89^Zr-ranibizumab was stable in serum for at least 24 h at 37°C (source of serum not mentioned).

For use as a control, a human immunoglobulin G (IgG) Fab fragment (size is comparable to ranibizumab and has no affinity for VEGF-A) was also labeled with ^89^Zr as described (7). The RY, RP, and SA of this labeled control were not reported.

^18^F-Fluorodeoxyglucose (^18^F-FDG) and [^18^O]H_2_O were produced for PET imaging as detailed elsewhere to compare PET images obtained with ^89^Zr-ranibizumab (7).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-ranibizumab%20in%20vitro%20studies&cmd=DetailsSearch)]

The percent binding of ^89^Zr-ranibizumab to VEGF was reported to be comparable to the unlabeled version of the mAb as determined with an enzyme-linked immunosorbent assay (7). The VEGF binding of the labeled mAb was shown to decrease with increasing concentrations of unlabeled ranibizumab.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-ranibizumab%20rodentia&cmd=DetailsSearch)]

The biodistribution of ^89^Zr-ranibizumab was studied in nude mice bearing SKOV-3 cell xenograft tumors as described by Nagengast et al. (7). Animals were injected with the radiolabeled mAb or with ^89^Zr-Fab-IgG through the penile vein. Mice were euthanized at 1, 3, 6, and 24 h p.i. (number of animals used per group was not reported), and radioactivity incorporated in the major organs, including tumors, was determined. Data were presented as percent of injected dose per gram tissue (% ID/g). With ^89^Zr-ranibizumab, the amount of radioactivity in the blood was shown to decrease from 8.44 ± 2.19% ID/g at 1 h p.i. to 0.38 ± 0.38% ID/g at 24 h p.i., indicating that there was a rapid clearance of the ^89^Zr from circulation. The amount of label detected in the heart, lung, liver, muscle, and bone was reported to be between ~1.0% ID/g (muscle) and ~5.0% ID/g (lungs) at 1 h p.i. and between ~0.5% ID/g (muscle) and ~4.0% ID/g (liver) at 24 h p.i. During the same period, the incorporation of radioactivity in the tumors from the labeled mAb increased from ~2.0% ID/g at 1 h p.i. to ~4.0% ID/g. With ^89^Zr-Fab-IgG, the amount of radioactivity in the tumor was reported to be ~1.5% ID/g at 24 h p.i. Increasing doses of unlabeled ranibizumab given to the mice were reported to decrease the tumor uptake of ^89^Zr-ranibizumab to the background levels observed with the radiolabeled Fab-IgG.

In another study, microPET imaging of mice bearing A2780 or Colo205 cell xenograft tumors (number of animals used per group was not reported) injected with either ^18^F-FDG or [^18^O]H_2_O (imaging performed at 1 h p.i.) or ^89^Zr-ranibizumab (imaging performed at 24 h p.i.) showed that the tumor could be clearly visualized on the animals with all the tracers (7). Treatment of the animals with sunitinib for a week followed by imaging showed that, in both cell type tumors, there was an ~45% and ~20% reduced uptake of the labeled mAb in the tumor center and the rim, respectively, compared with the tumor uptake in animals given no drug treatment. ^18^F-FDG imaging of animals treated the TK inhibitor showed that the label was present uniformly across the lesion; in imaging with ^18^O, only the tumor rim was clearly visible while the center was not visible. Compared with untreated mice, tumors on the sunitinib-treated animals showed a minimal change in uptake of the Fab-IgG. PET imaging in mice one week after stopping sunitinib treatment showed an increased tumor uptake of ^89^Zr-ranibizumab in both tumor models (7). The increase was ~70% and ~35% higher (P = 0.056) compared to the 7-day sunitinib treatment and the baseline, respectively. Histological staining of tumors obtained from the sunitinib-treated animals showed that there was increased vascularization and expression of VEGFR on the tumor rim compared with the tumor center; these studies also confirmed the differential uptake of ^89^Zr-ranibizumab observed at the tumor center and the rim during the PET imaging studies (7).

From these studies, the investigators concluded that PET imaging with ^89^Zr-ranibizumab is suitable to visualize and possibly quantify VEGF signaling in cancerous tumors and has a potential application to monitor anti-cancer therapy (7).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-ranibizumab%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-ranibizumab%20Non-Human%20Primates&cmd=DetailsSearch)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-ranibizumab%20Human%20Studies&cmd=DetailsSearch)]

No publications are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Jubb A.M., Harris A.L. (2010). Biomarkers to predict the clinical efficacy of bevacizumab in cancer. Lancet Oncol.
2 Roodink I., Leenders W.P. (2010). Targeted therapies of cancer: angiogenesis inhibition seems not enough. Cancer Lett.
3 Kourlas H., Abrams P. (2007). Ranibizumab for the treatment of neovascular age-related macular degeneration: a review. Clin Ther.
4 Niu G., Chen X. (2010). Vascular endothelial growth factor as an anti-angiogenic target for cancer therapy. Curr Drug Targets.
5 Nagengast W.B., de Vries E.G., Hospers G.A., Mulder N.H., de Jong J.R., Hollema H., Brouwers A.H., van Dongen G.A., Perk L.R., Lub-de Hooge M.N. (2007). In vivo VEGF imaging with radiolabeled bevacizumab in a human ovarian tumor xenograft. J Nucl Med.
6 Ferrara N., Damico L., Shams N., Lowman H., Kim R. (2006). Development of ranibizumab, an anti-vascular endothelial growth factor antigen binding fragment, as therapy for neovascular age-related macular degeneration. Retina.
7 Nagengast W.B., Lub-de Hooge M.N., Oosting S.F., den Dunnen W.F., Warnders F.J., Brouwers A.H., de Jong J.R., Price P.M., Hollema H., Hospers G.A., Elsinga P.H., Hesselink J.W., Gietema J.A., de Vries E.G. (2011). VEGF-PET imaging is a noninvasive biomarker showing differential changes in the tumor during sunitinib treatment. Cancer Res.